# Amine-modified silica-coated polyhedral superparamagnetic iron oxide nanoparticle–labeled rabbit bone marrow–derived mesenchymal stem cells

Chemical name: | Amine-modified silica-coated polyhedral superparamagnetic iron oxide nanoparticle–labeled rabbit bone marrow–derived mesenchymal stem cells
Abbreviated name: | SPIO@SiO_2_-NH_2_-labeled MSCs
Synonym:
Agent Category: | Cells
Target: | Others (cell imaging)
Target Category: | Non-targeted
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal / contrast: | SPIO
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=mesenchymal+stem+cells+and+cell+tracking+and+imaging)]

Personalized diagnosis and treatment with allogenic or autologous cells are becoming a reality in the field of medicine (1, 2). Cytotoxic or engineered T cells (http://clinicaltrials.gov/ct2/results?term=cytotoxic+T+cells) are under clinical trial for the treatment of hematopoietic or other malignant diseases (3). Contrast agent-tagged macrophages (http://clinicaltrials.gov/ct2/results?term=macrophage+and+imaging) are used as cellular probes to image the early inflammatory processes in macrophage-rich conditions such as inflammation, atherosclerosis, and acute cardiac graft rejection (4). The roles of stem cells (http://clinicaltrials.gov/ct2/results?term=stem+cell) are under intensive investigation in the therapeutic and regenerative medicine such as regenerating cardiomyocytes, neurons, bone, and cartilage (1). Genetically modified cells (http://clinicaltrials.gov/ct2/results?term=genetic+disorders+and+cells) are used to treat genetic disorders (5). With the promising results from these studies, a critical issue is how to monitor the temporal and spatial migration and the homing of these cells, as well as the engraftment efficiency and functional capability of the transplanted cells in vivo (6, 7). Histopathological techniques have only been used to obtain information on the fate of implanted cells at the time of animal euthanization or via biopsy or surgery. To track the real-time changes of cell location, viability, and functional status, cell imaging techniques have been introduced during the last few years. Cells of interest are labeled with reporter genes, fluorescent dyes, or other contrast agents that transform the tagged cells into cellular probes or imaging agents (2, 6, 7).

The ability to monitor superparamagnetic iron oxide particles (SPIO) by magnetic resonance imaging (MRI) has been utilized in animal models as well as in a few clinical settings to investigate the fate of labeled cells (6-9). The advantages of using MRI for cell tracking include the high spatial resolution with high anatomic background contrast, the lack of exposure to ionizing radiation, and the ability to follow the cells for months. SPIO particles provide a strong change in signal per unit of metal, in particular on T2-weight images. In addition, cell labeling with SPIO nanoparticles is generally nontoxic and does not affect the cell proliferation and differentiation capacity, although a few studies have reported that the stem cells labeled with SPIO lose part of their differentiation capacity in a SPIO concentration–dependent manner (10, 11). The important limitation of MRI is the fact that MRI signals cannot indicate whether cells are dead or alive. It is also unknown whether the MRI signal comes from targeted or labeled cells or from macrophages. Basically, SPIO particles are used to label the target cells by systemic application or by injecting into the tissue area of interest to monitor target cell migration after phagocytosis. SPIO are more frequently used to label the cells in vitro by incorporating into the cells directly. Furthermore, SPIO are usually encapsulated by organic polymers to increase their stability and bio-compatibility, and allow the chemical modification of their surfaces. The fact is that the uptake of different particles varies largely between different cell types (6, 7).

Mesenchymal stem cells (MSCs) represent a heterogeneous subset of pluripotent stromal cells that can be isolated from different adult tissues including adipose tissue, liver, muscle, amniotic fluid, placenta, umbilical cord blood, and dental pulp, although the bone marrow remains the principal source for most preclinical and clinical studies (1, 12, 13). Although MSCs account for only 0.01–0.001% of the total nucleated cells within isolated bone marrow aspirates, they can easily be isolated and expanded in vitro through as many as 40 population doublings in ~8–10 weeks of culture (1, 14). These cells exhibit the potential to differentiate into cells of diverse lineages, such as adipocytes, chondrocytes, osteocytes, myoblasts, cardiomyocytes, neurons, and astrocytes. In addition, MSCs possess remarkable immunosuppressive properties, and they have been shown to be effective against tumor cell growth (15, 16). Wang et al. developed amine-modified silica-coated polyhedral SPIO nanoparticles (SPIO@SiO_2_-NH_2_) for MRI real-time cell tracking of implanted MSCs (8). Using the nanoparticles, the investigators obtained a high labeling efficiency in labeling the rabbit bone marrow–derived MSCs, and they could monitor the labeled MSCs with MRI for up to 2–3 months in vivo.

### Relevant Resource Links

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=cell+tracking+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Mesenchymal stem cells under clinical trails (http://clinicaltrials.gov/ct2/results?term=mesenchymal+stem+cells)
- SPIO and cell imaging under clinical trails (http://clinicaltrials.gov/ct2/results?term=SPIO+and+cell+imaging)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=SPIO+and+silica+and+amine)]

Wang et al. described the synthesis procedure of SPIO@SiO_2_-NH_2_ in detail (8). They synthesized the polyhedral crystalline SPIO nanoparticles (6 nm in diameter) with co-precipitation of FeCl_3_ and FeSO_4_, followed by solvothermal treatment. The SPIO nanoparticles were then coated with a thin layer of silica with (SPIO@SiO_2_-NH_2_) or without (SPIO@SiO_2_) amine groups on the surface of the particles. SPIO@SiO_2_-NH_2_ and SPIO@SiO_2_ nanoparticles exhibited similar structural features except for their surface charges at certain pH values. Both were nearly monodispersed polyhedral crystals with an average diameter of 10.7 ± 2.6 nm for SPIO@SiO_2_-NH_2_ and 8.5 ± 3.0 nm for SPIO@SiO_2_. Under electron microscopy, the nanoparticles had a single iron oxide core with a single silica shell and were uniform in size. The iron contents of the SPIO@SiO_2_-NH_2_ and SPIO@SiO_2_ nanoparticles were 44.8 ± 0.2% and 21.6 ± 0.1%, respectively. The amounts of silicon, carbon, and nitrogen elements in the SPIO@SiO_2_-NH_2_ nanoparticles were 11%, 11%, and 5%, separately. The amine surface modification did not affect the original morphology or the crystallinity of the magnetite core. The saturation magnetizations were 52.5 and 43.5 emu/g Fe, and the MR relaxivities (r2) were 43.5 ± 9.1 and 18.9 ± 3.6 mmol^-1^s^-1^ for the SPIO@SiO_2_-NH_2_ and SPIO@SiO_2_ nanoparticles, respectively.

MSCs were isolated from the bone marrow of 20-week-old New Zealand white rabbits and expanded with culture for 5–7 days before labeling. To label the MSCs, Wang et al. tested different concentrations of the nanoparticles, different labeling times, and various transfection agents, and they determined the optimal condition of labeling as an iron concentration of 4.5 µg/ml, an incubation time of 16 h at ambient temperature, and no use of transfection agents. Transfection agents poly-L-lysine and lipofectamine 2000 did not increase the labeling efficiency. On the basis of Prussian blue staining, the labeling efficiency was close to 100%. The iron contents of the labeled MSCs for the SPIO@SiO_2_ and SPIO@SiO_2_-NH_2_ were 17.4 ± 3.9 and 68.7 ± 11.2 pg/cell, respectively, immediate after labeling, and these values decreased to 4.2 ± 1.5 and 13.7 ± 2.1 pg/cell, respectively, 33 days after labeling. The nanoparticles were located in the lysosomes and vesicles, and there were no nanoparticles in the nuclei or other structures up to 33 days after labeling.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=SPIO+and+silica+and+amine)]

Cell pellet MRI showed that a pellet with ≥5,000 SPIO@SiO_2_-labeled MSCs or with ≥1,000 SPIO@SiO_2_-NH_2_-labeled MSCs was detectable immediate after labeling, and increased to ≥5 × 10^4^ SPIO@SiO_2_-labeled MSCs or ≥10^4^ SPIO@SiO_2_-NH_2_-labeled MSCs on day 33 of culture after labeling. These results indicate that both SPIO@SiO_2_ and SPIO@SiO_2_-NH_2_ nanoparticles had durable MSC-labeling capacity under in vitro culture conditions in which very fast cell division usually occurs under the stimulus of fetal calf serum. The results also demonstrated that the surface amine modification enhanced the labeling efficiency. At physiological pH, SPIO@SiO_2_ nanoparticles were negatively charged, whereas SPIO@SiO_2_-NH_2_ nanoparticles were positively charged because of amine modification. The cell labeling enhancement was thought to be due to the electrostatic interaction between the positively charged SPIO@SiO_2_-NH_2_ and the negatively charged MSC cell membrane at physiological pH (8).

After cell labeling with the particles (iron concentration in medium, 4.5 µg/ml) for 16 h, cytotoxicity analysis with trypan blue showed that the cell viability was 95.7 ± 2% and 94.2 ± 3% after labeling with SPIO@SiO_2_ and SPIO@SiO_2_-NH_2_, respectively. MTT assessments before labeling and at 16 h and 120 h after labeling did not reveal altered cell proliferation capacity. The labeled MSCs retained the osteogenic, adipogenic, and chondrogenic differentiation potentials.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=SPIO+and+silica+and+amine)]

To test the feasibility of tracking MSCs with MRI, Wang et al. injected SPIO@SiO_2_-NH_2_-labeled MSCs into the right hemisphere (1 cm depth) of the New Zealand male white rabbits’ brain (1 × 10^5^ cells, n = 2) or into the left erector spinae muscle at a depth of 6 mm (5 × 10^4^ cells, n = 2) (1 × 10^7^ cells are commonly used for stem cell–based therapy in the clinical setting) (8). The first MRI was performed with a 3.0-T clinical whole-body MRI unit 2 days after MSC implantation, and then every 2 weeks until the eighth (n = 2) or twelfth week (n = 2). The parameters for imaging were described in detail by Wang et al. SPIO@SiO_2_-NH_2_-labeled MSCs induced decreased signal presenting as signal void areas at 2 days in the rabbit brain and in the erector spinae muscle. At 8 weeks, the signal void areas were still visible but became wider, indicating MSC migration. At 12 weeks, the signal void was still visible, but there was a strong decrease in the sizes of areas. Histological sections with Prussian blue staining suggested that the SPIO nanoparticles were predominantly located within the MSCs and MSC-derived cells. No apparent phagocytic cells existed at the implanted sites in either the brain or the erector spinae muscle. These results indicate that the SPIO@SiO_2_-NH_2_-labeled MSCs can be tracked with MRI for up to 3 months.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Mathiasen A.B., Haack-Sorensen M., Kastrup J. (2009). Mesenchymal stromal cells for cardiovascular repair: current status and future challenges. Future Cardiol.
2 Arbab A.S., Janic B., Haller J., Pawelczyk E., Liu W., Frank J.A. (2009). In Vivo Cellular Imaging for Translational Medical Research. Curr Med Imaging Rev.
3 Cesco-Gaspere M., Morris E., Stauss H.J. (2009). Immunomodulation in the treatment of haematological malignancies. Clin Exp Med.
4 Eisenblatter M., Ehrchen J., Varga G., Sunderkotter C., Heindel W., Roth J., Bremer C., Wall A. (2009). In vivo optical imaging of cellular inflammatory response in granuloma formation using fluorescence-labeled macrophages. J Nucl Med.
5 Bachoud-Levi A.C. (2009). Neural grafts in Huntington's disease: viability after 10 years. Lancet Neurol.
6 Himmelreich U., Dresselaers T. (2009). Cell labeling and tracking for experimental models using magnetic resonance imaging. Methods.
7 Hoehn M., Wiedermann D., Justicia C., Ramos-Cabrer P., Kruttwig K., Farr T., Himmelreich U. (2007). Cell tracking using magnetic resonance imaging. J Physiol.
8 Wang H.H., Wang Y.X., Leung K.C., Au D.W., Xuan S., Chak C.P., Lee S.K., Sheng H., Zhang G., Qin L., Griffith J.F., Ahuja A.T. (2009). Durable mesenchymal stem cell labelling by using polyhedral superparamagnetic iron oxide nanoparticles. Chemistry.
9 Yoon T.J., Kim J.S., Kim B.G., Yu K.N., Cho M.H., Lee J.K. (2005). Multifunctional nanoparticles possessing a "magnetic motor effect" for drug or gene delivery. Angew Chem Int Ed Engl.
10 Arbab A.S., Bashaw L.A., Miller B.R., Jordan E.K., Lewis B.K., Kalish H., Frank J.A. (2003). Characterization of biophysical and metabolic properties of cells labeled with superparamagnetic iron oxide nanoparticles and transfection agent for cellular MR imaging. Radiology.
11 Arbab A.S., Liu W., Frank J.A. (2006). Cellular magnetic resonance imaging: current status and future prospects. Expert Rev Med Devices.
12 Ehrchen J., Helming L., Varga G., Pasche B., Loser K., Gunzer M., Sunderkotter C., Sorg C., Roth J., Lengeling A. (2007). Vitamin D receptor signaling contributes to susceptibility to infection with Leishmania major. FASEB J.
13 Sadan O., Melamed E., Offen D. (2009). Bone-marrow-derived mesenchymal stem cell therapy for neurodegenerative diseases. Expert Opin Biol Ther.
14 Huang D.M., Hsiao J.K., Chen Y.C., Chien L.Y., Yao M., Chen Y.K., Ko B.S., Hsu S.C., Tai L.A., Cheng H.Y., Wang S.W., Yang C.S. (2009). The promotion of human mesenchymal stem cell proliferation by superparamagnetic iron oxide nanoparticles. Biomaterials.
15 Loebinger M.R., Kyrtatos P.G., Turmaine M., Price A.N., Pankhurst Q., Lythgoe M.F., Janes S.M. (2009). Magnetic resonance imaging of mesenchymal stem cells homing to pulmonary metastases using biocompatible magnetic nanoparticles. Cancer Res.
16 Kuhn N.Z., Tuan R.S. (2010). Regulation of stemness and stem cell niche of mesenchymal stem cells: implications in tumorigenesis and metastasis. J Cell Physiol.